# ^111^In-1,4,7,10-Tetraazacyclododecane-1,4,7-triacetic acid-L-homoalanine

Chemical name: | ^111^In-1,4,7,10-Tetraazacyclododecane-1,4,7-triacetic acid-L-homoalanine
Abbreviated name: | ^111^In-DO3A-H
Synonym:
Agent category: | Compound
Target: | L-type amino acid transporter 1 (LAT1)
Target category: | Neutral amino acid uptake
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DO3A-H)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain tissues (3). These amino acids are composed of naturally occurring amino acids, such as L-[^11^C]leucine, S-[^11^C]methyl-L-methionine ([^11^C]MET), and L-[^11^C]tyrosine, and of non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. ^123^I-Labeled amino acids are also used in oncological imaging (1, 4, 5).

Some 20 amino acid transporter systems have been identified (1). Most amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system, a Na-dependent transporter system A, or a Na^+^-dependent system B^0^ (6). They are retained in tumor cells due to their metabolic activities, including incorporation into proteins, which are higher than most normal cells (1). Malignant transformation increases the use of amino acids for energy, protein synthesis, and cell division. Tumor cells have been found to have overexpressed transporter systems (7). L-[^11^C]MET, [^18^F]fluorotyrosine, L-[^11^C]leucine, and [^18^F]fluoro-α-methyl tyrosine have been widely used in the detection of tumors (2, 6), but they are not approved by the United States Food and Drug Administration. These agents are moved into cells by various amino acid transporters and are incorporated into proteins. The fraction of radiolabeled amino acid that is incorporated into protein is usually small compared to the total amount taken up into the cell; leucine is an exception because it is quantitatively incorporated into proteins. The functions of these natural amino acid imaging agents are based on amino acid transport and protein incorporation.

Lee et al. (8) synthesized a series of ^111^In-labeled alanine and lysine derivatives of 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA), DO3A, and DO2A. Based on their in vitro cellular accumulation in tumor cells, ^111^In-1,4,7,10-tetraazacyclododecane-1,4,7-triacetic acid-L-homoalanine (^111^In-DO3A-H) was selected for use with in vivo single-photon emission computed tomography (SPECT) imaging studies in tumor-bearing nude mice.

### Related Resource Links:

- Chapters in MICAD (amino acid transporters (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D), homoalanine (http://www.ncbi.nlm.nih.gov/books?term=homoalanine%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (L-type amino acid transporter 1 (http://www.ncbi.nlm.nih.gov/gene/8140), L-type amino acid transporter 2 (http://www.ncbi.nlm.nih.gov/gene/23428), A-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/54407))
- Articles in Online Mendelian Inheritance in Man (OMIM) (amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters), L-[^11^C]methionine (http://www.clinicaltrials.gov/ct2/results?term=11C+MET))
- Drug information in FDA (amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15), L-[^11^C]methionine (http://google2.fda.gov/search?q=11C-methionine+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DO3A-H%20and%20synthesis)]

DO3A-H (5 nmol) was mixed with 7.4 MBq (0.2 mCi) ^111^InCl_3_ in 0.1 M sodium acetate buffer (pH 4.0) and incubated for 10 min at 95°C (8). The labeling efficiency of ^111^In incorporation was >96%. ^111^In-DOTA was prepared similarly as a control. ^111^In-DO3A-H and ^111^In-DOTA were found to be stable for 22 h in sodium bicarbonate buffer (pH 7) at room temperature and human serum at 37°C after incubation.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DO3A-H%20and%20in%20vitro)]

In vitro cellular accumulation studies (n = 3) were performed using human malignant glioma U87MG cells with ^111^In-DO3A-H and ^111^In-DOTA (8). At 10–90 min, ^111^In-DO3A-H showed higher cellular radioactivity (0.8–1.3% dose/mg protein (% D/g)) than ^111^In-DOTA (0.1–0.2% D/g). Cellular accumulation of ^111^In-DO3A-H radioactivity was reduced by exposure to 2-aminobicyclo[2.2.1]heptane-2-carboxylic acid (BCH, an L-type transporter inhibitor) in a dose-dependent manner (0.001–1.0 mM), whereas little dose-dependent inhibition was observed in the presence of N-methyl-α-aminoisobutyric acid (an A-type transporter inhibitor) and serine. Specific transport of ^111^In-DO3A-H in U87MG cells was mediated mainly by the L-type amino acid transporter.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DO3A-H%20and%20rodentia)]

Ex vivo biodistribution was studied in nude mice (n = 4/group) bearing U87MG xenografts at 10 min and 60 min after injection of 0.037 MBq (0.001 mCi) ^111^In-DO3A-H or ^111^In-DOTA (8). The tissue with the highest uptake at 10 min was the kidney (11% injected dose (ID)/g)) for both tracers with rapid clearance at 60 min for the kidney and other normal tissues. The tumor accumulation of radioactivity at 60 min was 1.10 ± 0.98% ID/g and 0.61 ± 0.22% ID/g for ^111^In-DO3A-H and ^111^In-DOTA, respectively. The tumor/muscle ratios at 60 min were 9.48 ± 8.47 and 5.61 ± 1.53 for ^111^In-DO3A-H and ^111^In-DOTA, respectively. No blocking studies were performed.

Lee et al. (8) performed whole-body SPECT imaging studies at 10–40 min after intravenous injection of 9.2 MBq (0.25 mCi) ^111^In-DO3A-H or ^111^In-DOTA in female nude mice (n = 4/group) bearing U87MG tumors. The tumor accumulation of radioactivity was visualized with ^111^In-DO3A-H but not with ^111^In-DOTA. High radioactivity was observed with both tracers in the urinary bladder. The tumor/muscle ratios at 40 min were 3.16 ± 0.74 and 1.8 ± 0.1 (P < 0.05) for ^111^In-DO3A-H and ^111^In-DOTA, respectively. Autoradiography with ^111^In-DO3A-H and immunohistochemistry analysis confirmed the localization of radioactivity to LAT1 in the tumor sections. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DO3A-H%20and%20%28pig%20or%20dog%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DO3A-H%20AND%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DO3A-H%20and%20human)]

[No publication is currently available.

## References

1 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
2 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
5 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
6 Langen K.J., Jarosch M., Muhlensiepen H., Hamacher K., Broer S., Jansen P., Zilles K., Coenen H.H. (2003). Comparison of fluorotyrosines and methionine uptake in F98 rat gliomas. Nucl Med Biol.
7 Saier M.H., Daniels G.A., Boerner P., Lin J. (1988). Neutral amino acid transport systems in animal cells: potential targets of oncogene action and regulators of cellular growth. J Membr Biol.
8 Lee J.J., Shetty D., Lee Y.S., Kim S.E., Kim Y.J., Hong M.K., Son J.Y., Jeong J.M. (2012). Evaluation of (111)In-labeled macrocyclic chelator-amino acid derivatives for cancer imaging. Nucl Med Biol.